# Anti-malondialdehyde-modified low-density lipoprotein MDA2 monoclonal antibody–labeled lipid-coated superparamagnetic iron oxide nanoparticles

Chemical name: | Anti-malondialdehyde-modified low-density lipoprotein MDA2 monoclonal antibody–labeled lipid-coated superparamagnetic iron oxide nanoparticles
Abbreviated name: | MDA2 LSPIOs
Synonym:
Agent category: | Antibody
Target: | Malondialdehyde-modified low-density lipoprotein (MDA-LDL)
Target category: | Antigen
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=44888831), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=217035086) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=338) for more information about apolipoprotein B.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide nanoparticles and other iron oxide formulations affect T2 primarily and lead to decreased signals. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

Apolipoprotein E (apoE) is essential for the normal catabolism of triglyceride-rich lipoprotein chylomicrons (lipoprotein particles) (2). Oxidation of low-density lipoprotein (LDL) generates a number of highly reactive short chain-length aldehydic fragments of oxidized fatty acids capable of conjugating with lysine residues of apoliprotein B and other proteins. Oxidized LDL is present in atherosclerotic lesions and is essential for formation of foam cells in atherosclerotic plaques. During atherogenic conditions, depositions of lipids and extracellular matrix proteins on the endothelial cell surfaces of the aorta and cells lead to the development of atherosclerotic plaques (3), which may erode and rupture. MDA2 is a murine monoclonal antibody to malondialdehyde-lysine epitopes of MDA-LDL and other oxidatively modified proteins but not to normal LDL (4). Briley-Saebo et al. (5) showed accumulation of MDA2 micelles containing Gd (MDA2-Gd micelles) in macrophages of atherosclerotic lesions in apoE-deficient (apoE^–/–^) mice using MRI. However, Gd may lead to renal toxicity in patients. In another study, Briley-Saebo et al. (6) conjugated MDA2 antibody to lipid-coated superparamagnetic iron oxide nanoparticles (LSPIOs) for in vivo detection of atherosclerotic lesions in apoE^–/–^ mice using MRI.

### Related Resource Links:

- Chapters in MICAD (MDA (http://www.ncbi.nlm.nih.gov/books?term=malondialdehyde%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (apolipoprotein E (http://www.ncbi.nlm.nih.gov/gene/348))
- Articles in Online Mendelian Inheritance in Man (OMIM) (apolipoprotein E (http://omim.org/entry/107741))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+synthesis)]

LSPIOs were prepared by incubation of oleic acid–coated iron oxide nanoparticles (magnetite) with 1,2-distearoyl-sn-glycer-3-phosphoethanolamine-n-methoxy(polyethylene glycol-2000 (PEG-DSPE) and PEG-malamide-DSPE (17.3 mg:1.3 mg per mg Fe) in a chloroform solution, with rhodamine added as a fluorescent label (6). The solution was added stepwise to boiling HEPES buffer (pH 7) under vigorous stirring until a clear brown solution was formed. LSPIOs were isolated with ultracentrifugation. MDA2 (2.3 nmol/mg Fe) was modified with S-acetylthioglycolic acid N-hydroxysuccinimide ester and then covalently linked to the surface of LSPIOs. MDA2 LSPIOs have a hydrated diameter (HD) of 38 ± 4 nm with an r1 value of 11 nM^–1^s^–1^ and an r2 value of 117 nM^–1^s^–1^ at 60 MHz and 40ºC. Untargeted LSPIOs have a HD of 35 ± 5 nm with an r1 value of 12 nM^–1^s^–1^ and an r2 value of 103 nM^–1^s^–1^ at 60 MHz and 40ºC. Only one in every sixteen LSPIOs contained an MDA2 antibody. MDA2 LSPIOs exhibited <5% variation in size and/or r2/r1 values at 4°C for 30 d.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+in+vitro)]

Confocal microscopy analysis showed accumulation of MDA2 LSPIOs (1 mM Fe in the extracellular solution) in MDA-LDL–pretreated J7774A.1 macrophages, whereas no accumulation (non-detectable) was observed with untargeted LSPIOs (1 mM Fe concentration) (6). The Fe content was 0.4 pg/cell for MDA2 LSPIOs and non-detectable for untargeted LSPIOs. The accumulation of dextran-coated Feridex (positive untargeted control, HD = 40 nm) by the macrophages was 1.9 pg Fe/cell; thus, the lipid-coating of LSPIOs limited their accumulation by the macrophages. If every MDA2-LSPIO contained MDA2 antibody, but only 1 in 16 did, a theoretical Fe accumulation of 5–6 pg Fe/cell was expected.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+rodentia)]

Briley-Saebo et al. (6) performed in vivo T2* MRI (9.4 T) studies of MDA2 LSPIOs in 10-month-old apoE^–/–^ knockout mice that were fed a high-fat, high-cholesterol diet at 6 weeks of age and 10-month-old wild-type normal mice on normal diet at 0 h and 24 h after intravenous injection. Animals were injected with either 3.9 mg Fe/kg MDA2 LSPIOs (n = 9 apoE^–/–^ mice or 5 wild-type mice) or LSPIOs (n = 5 apoE^–/–^ mice or 5 wild-type mice). There was a small loss (~10%) of R2* value in the apoE^–/–^ with MDA2 LSPIOs and little loss of R2* signal with untargeted LSPIOs in the atherosclerotic lesions. The liver accumulations were 37% and 35% injected dose for MDA2 LSPIOs and LSPIOs, respectively. The blood half-lives were 7.28 h and 1.02 h for MDA2 LSPIOs and LSPIOs in apoE^–/–^ mice, respectively. On the other hand, the blood half-lives (1.12 h versus 1.01 h) were similar in the wild-type mice. A similar loss (10%–15%) of R2* signal was also observed with a human single-chain Fv antibody fragment IK17 targeted to MDA-like epitopes (IK17-LSPIOs) and a natural IgM autoantibody (E06) cloned from apoE^–/–^ mice that binds to the phosphocholine head group of oxidized phospholipids (E06-LSPIOs). The investigators suggested that the LSPIOs are too large to allow for optimal diffusion into the atherosclerotic lesions. On the other hand, the use of lipid-coated ultra-small superparamagnetic iron oxide nanoparticles conjugated with MDA2 (MDA2 LUSPIOs, HD = 14 ± 3 nm) showed a significant (P < 0.003) loss of R2* signal in the atherosclerotic lesions in apoE^–/–^ mice. Co-injection of 20 nmol MDA2 antibody inhibited the loss of R2* value by 75% (P < 0.0002).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+human)]

No publication is currently available.

## NIH Support

R01 EB009638, R01 EB009638-07, R01 HL071021-07, R01 HL078667-04S1, R01 HL71021, R01 HL78667, R21 HL091399-01A2, R21 HL091399-02

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Eichner J.E., Dunn S.T., Perveen G., Thompson D.M., Stewart K.E., Stroehla B.C. (2002). Apolipoprotein E polymorphism and cardiovascular disease: a HuGE review. Am J Epidemiol.
3 Libby P. (2002). Inflammation in atherosclerosis. Nature.
4 Palinski W., Yla-Herttuala S., Rosenfeld M.E., Butler S.W., Socher S.A., Parthasarathy S., Curtiss L.K., Witztum J.L. (1990). Antisera and monoclonal antibodies specific for epitopes generated during oxidative modification of low density lipoprotein. Arteriosclerosis.
5 Briley-Saebo K.C., Shaw P.X., Mulder W.J., Choi S.H., Vucic E., Aguinaldo J.G., Witztum J.L., Fuster V., Tsimikas S., Fayad Z.A. (2008). Targeted molecular probes for imaging atherosclerotic lesions with magnetic resonance using antibodies that recognize oxidation-specific epitopes. Circulation.
6 Briley-Saebo K.C., Cho Y.S., Shaw P.X., Ryu S.K., Mani V., Dickson S., Izadmehr E., Green S., Fayad Z.A., Tsimikas S. (2011). Targeted iron oxide particles for in vivo magnetic resonance detection of atherosclerotic lesions with antibodies directed to oxidation-specific epitopes. J Am Coll Cardiol.